# ^123^I-Arg-Glu-Asn-Leu-Arg-Ile-Ala-Leu-Arg-Tyr

Chemical name: | ^123^I-Arg-Glu-Asn-Leu-Arg-Ile-Ala-Leu-Arg-Tyr
Abbreviated name: | ^123^I-B2702-p
Synonym: | ^123^I-RENLRIALRY
Agent Category: | Peptide
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target Category: | Receptor binding
Method of detection: | SPECT, gamma planar imaging
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=B2702-p)]

Endothelial cells are important cells in inflammatory responses (1, 2). Bacterial lipopolysaccharides (LPS), viruses, inflammation, and tissue injury increase secretion of tumor necrosis factor-α (TNF-α), interleukin-1 (IL-1), and other cytokines and chemokines. Emigration of leukocytes from blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (3).

VCAM-1 is found in very low levels (often non-detectable) on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (4-8). VCAM-1 binds to its counterligand integrin, very late antigen-4 (VLA-4), on the cell surface of leukocytes. Inflammatory cytokines, such as IL-1 and TNF-α, increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression was also induced by oxidized low-density lipoproteins under atherogenic conditions (1). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression toward vulnerable plaques, which may erode and rupture. A synthetic peptide (Arg-Glu-Asn-Leu-Arg-Ile-Ala-Leu-Arg-Tyr, B2702-p) corresponding to residues 75–84 of HLA-B2702 was shown to bind specifically to VCAM-1 (9). ^123^I-Labelingof B2702-p was performed on the tyrosine (residue 84) using the chloramine-T method (10). ^123^I-labeled B2702-p is being developed as a non-invasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=B2702-p+and+synthesis)]

B2702-p (prepared by solid-phase synthesis) was labeled with sodium [^123^I]iodide by electrophilic radioiodination using the chloramine-T method (10). A total of 200 MBq (5.41 mCi) ^123^I was added to 20–40 nmol B2702-p in the presence of 20–80 μg chloramine T. The reaction was stopped after 15 min. ^123^I-B2702-p was purified by anion exchange column chromatography. No yield, specific activity, or radiochemical purity values were reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=B2702-p+and+in+vitro)]

Fluorescence polarization experiments estimated a K_d_ value of 270 nM for the interaction between VCAM-1 and B2702-p (10).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=B2702-p+and+rodentia)]

Broisat et al. (10) reported studies of ^123^I- or ^99m^Tc-labeled B2702-p uptake into aortas of Watanabe heritable hyperlipidemic (WHHL) rabbits (n = 6) and control animals (n = 6) by ex vivo autoradiographic imaging, gamma counting, VCAM-1 immunohistology, and Sudan IV lipid staining at 180 min after injection. Robust VCAM-1 immunostaining was observed in Sudan IV–positive and to a lesser extent in Sudan IV–negative areas of WHHL rabbits, whereas no expression was detected in control rabbits. ^123^I-B2702-p exhibited a 2.9-fold increase in aortic/blood ratios between WHHL and control rabbits (P < 0.05), whereas ^99m^Tc-B2702-p showed a 1.9-fold increase (P < 0.05). Both tracer uptakes on ex vivo images co-localized with atherosclerotic plaques. Image quantification indicated a graded increase in ^123^I-B2702-p and ^99m^Tc-B2702-p activities from control to Sudan IV–negative and to Sudan IV–positive areas, correlating to the observed pattern of VCAM-1 expression. Sudan IV–positive tracer activity to control area tracer activity ratios were 17.0 ± 9.0 and 5.9 ± 1.8 for ^123^I-B2702-p and ^99m^Tc-B2702-p, respectively. No significant difference was observed in ^123^I-B2702-p and ^99m^Tc-B2702-p radioactivity between control and WHHL rabbits in all other organs examined. The kidneys (0.307 ± 0.052 versus 0.490 ± 0.184) and lungs (0.138 ± 0.028 versus 0.163 ± 0.044) were the major organs for ^123^I-B2702-p accumulation, whereas the kidneys (0.558 ± 0.109 versus 1.361 ± 0.721), livers (0.427 ± 0.080 versus 0.332 ± 0.042), and lungs (0.166 ± 0.052 versus 0.208 ± 0.044) were the major organs for ^99m^Tc-B2702-p accumulation. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=B2702-p+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=B2702-p+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=B2702-p+and+human)]

No publication is currently available.

## References

1 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
2 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
3 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
4 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
5 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
6 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
7 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
8 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
9 Ling X., Tamaki T., Xiao Y., Kamangar S., Clayberger C., Lewis D.B., Krensky A.M. (2000). An immunosuppressive and anti-inflammatory HLA class I-derived peptide binds vascular cell adhesion molecule-1. Transplantation.
10 Broisat A., Riou L.M., Ardisson V., Boturyn D., Dumy P., Fagret D., Ghezzi C. (2007). Molecular imaging of vascular cell adhesion molecule-1 expression in experimental atherosclerotic plaques with radiolabelled B2702-p. Eur J Nucl Med Mol Imaging.